# 3-β-(4-Iodophenyl)tropane-2-β-carboxylic acid 2-[^18^F]fluoroethyl ester

Chemical name: | 3-β-(4-Iodophenyl)tropane-2-β-carboxylic acid 2-[^18^F]fluoroethyl ester
Abbreviated name: | [^18^F]FE@CIT
Synonym:
Agent Category: | Compound
Target: | Dopamine transporter
Target Category: | Binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE@CIT)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion. Parkinson’s disease (PD) is associated with a loss of dopamine-containing neurons in the striatum, resulting in a loss of dopamine transporters (DAT) in the presynaptic nerve terminals (1, 2). Reduced DAT density is inversely correlated with the severity of motor dysfunction in PD patients. Several cocaine analogs have been developed for the evaluation of DAT density in the neurons of PD patients. Radiolabeled 2-β-carboxymethoxy-3-β-(4-iodophenyl)tropane (β-CIT) and N-(3-fluoropropyl)-2β-carbomethoxy-3β-(4-iodophenyl)nortropane (FP-CIT) have been used for brain imaging (3-6). Because of the short physical half-life of ^11^C-labeled analogs, equilibrium conditions are difficult to achieve in positron emission tomography (PET) measurements. [^123^I]β-CIT was studied with single-photon emission computed tomography (SPECT), which showed slow tracer uptake kinetics (7, 8). This led to the development of 3-β-(4-iodophenyl)tropane-2-β-carboxylic acid 2-[^18^F]fluoroethyl ester ([^18^F]FE@CIT) for PET brain imaging in PD patients (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE@CIT%20AND%20synthesis)]

[^18^F]FE@CIT was synthesized by reaction of 3-β-(4-iodophenyl)tropane-2-β-carboxylic acid with 2-bromo-1-[^18^F]fluoroethane ([^18^F]BFE) for 20 min at 150°C (9). [^18^F]BFE was prepared by nucleophilic fluorination of 2-bromoethyl triflate using the standard [^18^F]KF Kryptofix complex for 10 min at 100°C. The radiochemical yields of [^18^F]FE@CIT were >90% (based on [^18^F]BFE) with a radiochemical purity of >99% and specific activity of >416 GBq/µmol (11.2 Ci/µmol) at the end of synthesis.

## In Vitro studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE@CIT%20AND%20in%20vitro)]

In vitro [^18^F]FE@CIT autoradiography of frozen brain sections obtained from rats was performed by Ettlinger et al. (10) The striatum exhibited a higher radioactivity level than the cortex. Gu et al. (11) showed that binding affinities (K_i_) of FE@CIT at DAT, serotonin transporter (SERT), and norepinephrine transporter (NET) were 0.93, 4.02, and 116 nM, respectively. FE@CIT exhibited a higher DAT affinity than FP-CIT for DAT (8.29 nM) and more selective affinity for DAT over SERT and NET.

## Animal Studies

### Rodents

[PubMed] (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE@CIT%20AND%20rodentia)

Mitterhauser et al. (9) performed biodistribution studies in rats (n = 4/group) at 5, 15, 30, 60, and 120 min after injection of 1.25–2.23 MBq (0.033–0.06 mCi). At 60 min after injection, the radioactivity in the striatum was 1.23% injected dose/g (ID/g), which was greater than the thalamus (0.42% ID/g) and cerebellum (0.33% ID/g). The highest striatum/cerebellum ratio was 3.73, and the highest thalamus/cerebellum ratio was 1.65. The other organs with high accumulation were the kidney (3.86% ID/g), liver (3.06% ID/g), and lung (0.86% ID/g), whereas the bowels (0.54% ID/g), bone (0.14% ID/g), blood (0.15% ID/g), and muscle (0.16% ID/g) exhibited little or low accumulation at 60 min. There were continuous increases in radioactivity in the kidneys and liver from 5 min to 120 min. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FE%40CIT+AND+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE@CIT%20AND%20monkeys)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE@CIT%20AND%20human)]

No publication is currently available.

## Human Studies

MH34006, MH47370, NS40587

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Abi-Dargham A., Gandelman M.S., DeErausquin G.A., Zea-Ponce Y., Zoghbi S.S., Baldwin R.M., Laruelle M., Charney D.S., Hoffer P.B., Neumeyer J.L., Innis R.B. (1996). SPECT imaging of dopamine transporters in human brain with iodine-123-fluoroalkyl analogs of beta-CIT. J Nucl Med.
4 Chaly T., Dhawan V., Kazumata K., Antonini A., Margouleff C., Dahl J.R., Belakhlef A., Margouleff D., Yee A., Wang S., Tamagnan G., Neumeyer J.L., Eidelberg D. (1996). Radiosynthesis of [18F] N-3-fluoropropyl-2-beta-carbomethoxy-3-beta-(4-iodophenyl) nortropane and the first human study with positron emission tomography. Nucl Med Biol.
5 Kazumata K., Dhawan V., Chaly T., Antonini A., Margouleff C., Belakhlef A., Neumeyer J., Eidelberg D. (1998). Dopamine transporter imaging with fluorine-18-FPCIT and PET. J Nucl Med.
6 Lundkvist C., Halldin C., Ginovart N., Swahn C.G., Farde L. (1997). [18F] beta-CIT-FP is superior to [11C] beta-CIT-FP for quantitation of the dopamine transporter. Nucl Med Biol.
7 Ishikawa T., Dhawan V., Kazumata K., Chaly T., Mandel F., Neumeyer J., Margouleff C., Babchyck B., Zanzi I., Eidelberg D. (1996). Comparative nigrostriatal dopaminergic imaging with iodine-123-beta CIT-FP/SPECT and fluorine-18-FDOPA/PET. J Nucl Med.
8 Laruelle M., Wallace E., Seibyl J.P., Baldwin R.M., Zea-Ponce Y., Zoghbi S.S., Neumeyer J.L., Charney D.S., Hoffer P.B., Innis R.B. (1994). Graphical, kinetic, and equilibrium analyses of in vivo [123I] beta-CIT binding to dopamine transporters in healthy human subjects. J Cereb Blood Flow Metab.
9 Mitterhauser M., Wadsak W., Mien L.K., Hoepping A., Viernstein H., Dudczak R., Kletter K. (2005). Synthesis and biodistribution of [18F]FE@CIT, a new potential tracer for the dopamine transporter. Synapse.
10 Ettlinger D.E., Hausler D., Wadsak W., Girschele F., Sindelar K.M., Mien L.K., Ungersbock J., Viernstein H., Kletter K., Dudczak R., Mitterhauser M. (2008). Metabolism and autoradiographic evaluation of [(18)F]FE@CIT: a Comparison with [(123)I]beta-CIT and [(123)I]FP-CIT. Nucl Med Biol.
11 Gu X.H., Zong R., Kula N.S., Baldessarini R.J., Neumeyer J.L. (2001). Synthesis and biological evaluation of a series of novel N- or O-fluoroalkyl derivatives of tropane: potential positron emission tomography (PET) imaging agents for the dopamine transporter. Bioorg Med Chem Lett.